# Cys-Arg-Pro-Pro-Arg-[^18^F]fluorodipalmitin-liposomes

Chemical name: | Cys-Arg-Pro-Pro-Arg-[^18^F]Fluorodipalmitin-liposomes
Abbreviated name: | CRPPR-[^18^F]FDP-liposomes
Synonym: | Cys-Arg-Pro-Pro-Arg-3-[^18^F]fluoro-1,2-dipalmitoyl glycerol-liposomes
Agent Category: | Compound
Target: | Unknown, heart
Target Category: | Binding
Method of detection: | PET
Source of signal/contrasat: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CRPPR)]

Endothelial cells are important in inflammatory responses (1, 2). The presence of bacterial lipopolysaccharide (LPS), virus growth, inflammation, and tissue injury increase secretion of tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokines and chemokines. Emigration of leukocytes from the blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells, and they also increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1, vascular cell adhesion molecule-1, integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movement of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (3).

Liposomes are double-membrane lipid vesicles (4). They have been widely studied as important carriers in controlling the spatial and temporal distribution of drug molecules or other bioactive molecules for targeted therapy; for example, they have been used as universal carriers of tumor chemotherapeutic agents, as antigen carriers to stimulate immune response, as carriers of nucleic acid for gene therapy, and as carriers of antibiotics for infectious disease treatment (5). Marik et al. (6) developed liposomes by incorporation of [^18^F]fluorodipalmitin ([^18^F]FDP) into the phospholipid bilayer to minimize internalization and metabolism in cells. Therefore, the images obtained using [^18^F]FDP-liposomes could be more reflective of the biodistribution of long-circulating liposomes. The linear peptide Cys-Arg-Pro-Pro-Arg (CRPPR) has been found to specifically bind to heart endothelium using phage display screenings. Zhang et al. (7) coupled polyethylene glycol-stearic acid to CRPPR to form the lipo-PEG-CRPPR peptide (LPP), which was later incorporated into [^18^F]FDP-liposomes. The resulting CRPPR-[^18^F]FDP-liposomes were found to home to mouse hearts as determined with dynamic positron emission tomography.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CRPPR+synthesis)]

CRPPR was prepared by standard solid-phase synthesis (7). Polyethylene glycol (PEG; molecular weight, 1,200 (m = 1), 2,400 (m = 2), or 3,600 Da (m = 3)) was coupled onto the peptidyl resin followed by Fmoc-Lys(Fmoc)-OH and stearic acid. LLP was cleaved from the resin and purified with high-performance liquid chromatography with a 20% yield. LLP was dimerized in 0.01 M ammonium bicarbonate. [^18^F]FDP was synthesized via nucleophilic substitution of the p-toluenesulfonyl moiety of 3-tosyl-1,2-dipalmitoyl glycerol with [^18^F]F^–^ as reported previously (6). [^18^F]KF/Kryptofix 2.2.2/K_2_CO_3_ and 3-tosyl-1,2-dipalmitoyl glycerol were heated in acetonitrile to 100°C for 20 min with a decay-corrected yield of 43 ± 10% (n = 12). [^18^F]FDP was purified with chromatography and exhibited a radiochemical purity of 99%, a total synthesis time of 60 min, and a specific activity >111 GBq/mmol (3 Ci/mmol). Long-circulating radiolabeled PEG-coated liposomes were prepared by adding a CH_2_Cl_2_ solution of [^18^F]FDP to a mixture of dimerized LLP, 1,2-dipalmitoyl-sn-glycero-3-phosphocholine (DPPC), and 1,2-distearoyl-sn-glycero-3-phosphoethanolamine-N-[methoxy(PEG)-2000] (DSPE-PEG2000) (7). After evaporation of the solvent, phosphate-buffered saline (PBS) was added to the residue and sonicated at 60°C for 1 min. The CRPPR-[^18^F]FDP-liposomes were purified with gel filtration. The size of CRPPR-3-[^18^F]FDP-liposomes was 110 ± 38 nm with a molar ratio of CRPPR-3:DSPE-PEG2000:DPPC (6%:6%:88%). Radiochemical yield and specific activity of CRPPR-3-[^18^F]FDP-liposomes were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CRPPR+and+in+vitro)]

Flow cytometry analysis showed that both endothelial and melanoma cells incubated with CRPPR-3-liposomes containing calcein exhibited higher fluorescence intensity than cells incubated with non-targeted liposomes (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CRPPR+rodentia)]

Zhang et al. (7) performed positron emission tomography imaging with [^18^F]FDP-liposomes and CRPPR-3-[^18^F]FDP-liposomes in normal mice (n = 4) for 90 min after injection. CRPPR-3-[^18^F]FDP-liposomes exhibited a high level of radioactivity in the heart (peak 39% injected dose (ID)/cc) and a lower level of radioactivity in the liver (peak 30% ID/cc), followed by the spleen (peak 27% ID/cc) and urinary bladder (4% ID/cc at 90 min). Radioactivity levels in the heart remained almost constant during the 90-min scan. The rapid blood clearance pattern exhibited a two-phase cycle with a half-life of 3.2 min during the distribution phase and a half-life of 78.7 min during the elimination phase. Other tissues cleared the radioactivity gradually except for the urinary bladder, which exhibited a gradual increase. Little radioactivity was detected in the bones and gut. The heart/muscle ratio was 32. Ex vivo autoradiography and confocal microscopy confirmed binding of CRPPR-3-[^18^F]FDP-liposomes to blood vessels within the heart. Pre-administration of polyinosinic acid (a scavenger receptor inhibitor) and CRPPR decreased the accumulation in the heart by 41% (P < 0.05) and 19% (P < 0.05) at 90 min, respectively. On the other hand, [^18^F]FDP-liposomes remained in the blood volume and were visualized in the heart chamber and carotid vessels. The [^18^F]FDP-liposome accumulation in the liver (peak 11% ID/cc) and spleen (peak 10% ID/cc) was less than that of the CRPPR-3-[^18^F]FDP-liposomes. On the other hand, biodistribution studies showed that the organ with the highest accumulation of CRPPR-3-[^18^F]FDP-liposomes was the heart (44% ID/g), followed by the liver (22% ID/g) and spleen (12% ID/g) 90 min after injection. The urine showed a radioactivity level of ~20% ID/g. Both [^18^F]FDP-liposomes and c(RGDY(OMe)KE)-[^18^F]FDP-liposomes (controls) remained in the blood circulation (>25% ID/g) with low radioactivity accumulation in the heart muscle (<4% ID/g), liver (<4% ID/g), and urine (<10% ID/g).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CRPPR+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CRPPR+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CRPPR+human)]

No publication is currently available.

## NIH Support

R01 CA103828, R24 CA110804

## References

1 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
2 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
3 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
4 Torchilin V.P. (1996). Liposomes as delivery agents for medical imaging. Mol Med Today.
5 Torchilin V.P. (2007). Targeted pharmaceutical nanocarriers for cancer therapy and imaging. Aaps J.
6 Marik J., Tartis M.S., Zhang H., Fung J.Y., Kheirolomoom A., Sutcliffe J.L., Ferrara K.W. (2007). Long-circulating liposomes radiolabeled with [18F]fluorodipalmitin ([18F]FDP). Nucl Med Biol.
7 Zhang H., Kusunose J., Kheirolomoom A., Seo J.W., Qi J., Watson K.D., Lindfors H.A., Ruoslahti E., Sutcliffe J.L., Ferrara K.W. (2008). Dynamic imaging of arginine-rich heart-targeted vehicles in a mouse model. Biomaterials.